# [^18^F]Fluoroerythronitroimidazole

Chemical name: | 4-[^18^F]Fluoro-2,3-dihydroxy-1(2’-nitro-1’imidazolyl)butane
Abbreviated name: | [^18^F]FETNIM
Synonym: | [^18^F]Fluoroerythronitroimidazole
Agent Category: | Compound
Target: | Hypoxic cells (macromolecules)
Target Category: | Intracellular reduction and binding
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Other non-primate mammals; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22fluoroerythronitroimidazole%22%5BSubstance%20Name%5D%20OR%20FETNIM%5BText%20Word%5D)]

Hypoxia in malignant tumors can be a major factor limiting the efficacy of radiotherapy and may also be a predictive factor for the occurrence of metastatic disease. This is the reason for a multitude of efforts to develop methods and imaging techniques for measuring oxygen in tissues. Methods for measuring tumor hypoxia use diverse technologies including biological, chemical and physical methods. Nitroimidazoles, used in conjunction with positron emission tomographic imaging (PET), offer a less invasive and less technically demanding alternative to the Eppendorf (oxygen) electrode method.

Nitroimidazoles are reduced intracellularly in cells. In aerobic cells, the reduced nitroimidazole is immediately reoxidised and washed out rapidly. On the other hand, an environment of low oxygen concentration induces further reductive reactions that ultimately lead to the formation of either reactive products that are able to covalently bind to cell components, or charged species that diffuse slowly out of the tissues (1). The bioreductive metabolism of 2-nitroimidazoles leads to nitroso (2e-), hydroxylamine (4e-), and amine (6e-) derivatives. When the fragmentation of the imidazole ring occurs, reactive portions of the molecule, such as glyoxal, bind to macromolecular components of cells in tissues and tumors (2)

Initial development of nitroimidazoles for in vivo imaging used radiohalogenated derivatives of misonidazole, some of which have been used in patients. Fluoromisonidazole ([^18^F]FMISO) is the most widely used nitroimidazole derivate for imaging hypoxia using PET. The two main problematic issues with [^18^F]FMISO are: i) its relatively low concentration within the lesion, ii) the need to wait several hours to allow clearance of the agent from the normoxic background tissue (contrast between lesion and background is typically < 2:1 at about 90 min after injection). Even with PET, this combination of circumstances can make successful evaluation of hypoxic lesions a challenge.

[^18^F]Fluoroerythronitroimidazole ([^18^F]FETNIM) is a novel imaging agent currently under investigation for the in vivo detection of tumor hypoxia using PET. [^18^F]FETNIM is more hydrophilic than [^18^F]FMISO, and therefore can be eliminated more rapidly from well-oxygenated tissues, allowing a higher tumor-to-background ratio. Preliminary research has shown that [^18^F]FETNIM has a slow peripheral metabolism, little defluorination, and trapping in hypoxic tumor tissue. But despite encouraging results, further studies need to be performed to justify the development of [^18^F]FETNIM-PET on a larger scale as a non-invasive assessment method for tumor hypoxia.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%22fluoroerythronitroimidazole%22%5BSubstance%20Name%5D%20OR%20FETNIM%5BText%20Word%5D%29%20AND%20synthesis%5BAll%20Fields%5D)]

The synthesis of [^18^F]FETNIM was first described by Yang et al. (3) in 1995. In the reported method, [^18^F]FETNIM is synthesized from the precursor 1-(2’-nitro-1’-imidazolyl)-2,3-O-isopropylidene-4-tosyloxybutane by nucleophilic displacement of the tosyloxy group with [^18^F]Fluoride followed by acidic hydrolysis of the diol-protecting group.

A slightly modified method proposed in 2001 by Grönroos et al. (4) consists of the following steps: After producing [^18^F]Fluoride by bombarding ^18^O-enriched water using a cyclotron, the target water is removed by azeotropic distillation with acetronitrile under reduced pressure, the tosylate is dissolved in dry acetonitrile and [^18^F]Fluoride/Kryptofix 222/K^+^ complex and heated for 8 min at 90 ºC. Hydrochloric acid (2mol/L) is then added to the dry residue, and a hydrolysis performed at 90 ºC for 2 min. After cooling, 2N NaOH is added and the mixture is then filtered and injected onto a HPLC column. After elution with a saline solution containing 2% ethanol (pH adjusted at 4.7), the fraction containing [^18^F]FETNIM is eluted for 13 min. and collected.

The entire synthetic procedure can be completed in 50 min. The radiochemical purity obtained is ≥ 95%, the radiochemical yields (corrected for decay) range between 13 and 20%, with an associated specific activity of c.a. 330 GBq/μmol.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fluoroerythronitroimidazole%20AND%20in%20vitro)]

No publication currently available

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%22fluoroerythronitroimidazole%22%5BSubstance%20Name%5D%20OR%20fluoroerythronitroimidazole%5BText%20Word%5D%29%20AND%20%22rodentia%22%5BMeSH%20Terms%5D)]

Biodistribution studies of [^18^F]FETNIM were performed on 20 female Sprague-Dawley rats bearing multiple mammary tumors (4). Two sets of studies were performed: a first one using [^18^F]FETNIM injected doses of 8.5 ± 2.2MBq (0.23 ± 0.06mCi) for data recorded at 15, 30 and 60 min after intravenous injection of the radiotracer; the second one using [^18^F]FETNIM injected doses of 50 ± 10 MBq (1.35 ± 0.27 mCi) for data recorded at 120 and 240 min. The highest tumor-to-blood radioactivity ratio was observed at 120min (1.79 ± 0.64 SD); it remained constant thereafter until 240 min. The organ showing the highest uptake at 120 min was the kidney (0.397 ± 0.092% ID/g tissue), while the lowest uptake was observed in the cerebellum (0.063 ± 0.009%ID/g). The bone uptake measured by Grönroos et al. (4) (0.058 ± 0.007% ID/g tissue) showed only a minimal defluorination. On the other hand, a high uptake in the bone marrow (0.37 ± 0.07% ID/g tissue) was observed at 1h post-injection.

[^18^F]FETNIM showed a much lower liver uptake (1.68 ± 0.62 liver-to-blood ratio) than reported by Rasey et al. for [^18^F]FMISO-PET (5). One should keep in mind though, that direct comparisons are often difficult to establish and to rely on, when studies are performed using different imaging protocols or methods of analysis.

Chung et al. (6) evaluated the tumor uptake of both [^18^F]Flurorodeoxyglucose ([^18^F]FDG) and [^18^F]FETNIM in male ICR mice bearing sarcoma 180 cell line xenografts. Radiotracers were injected intravenously (185 kBq); the tumors used in the experiments weighed 0.26 - 5.82 g. For both radiotracers, the tumor uptake (per-gram radiotracer) was inversely proportional to the tumor weight, but also depended on the distribution of necrosis. The tumor uptake values reported for [^18^F]FETNIM and [^18^F]FDG were 1.77 ± 0.48% ID/g and 6.27 ± 2.53% ID/g, respectively. [^18^F]FETNIM showed a closer correlation (r = -0.593, p < 0.05) than [^18^F]FDG (r = -0.447, p < 0.05) and was found to accumulate in both viable and partially necrotic areas. ([^18^F]FDG accumulated in viable areas only).

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FETNIM%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FETNIM%20AND%20%28dog%20OR%20pig%20OR%20sheep%29)]

Very limited investigations on non-primate mammals have been performed so far. [^18^F]FETNIM-PET studies by Grönroos et al. (4) on rats and dogs (using radio-TLC analyses) showed that the amount of unchanged [^18^F]FETNIM in dog venous plasma remained constant at 86% ± 4% over a 90 min dynamic scan, and that the binding of [^18^F]FETNIM was minimal. The reported average amount of unbound [^18^F]FETNIM in dogs was 95% ± 5% (for a 5-90 min period of time post-injection.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fluoroerythronitroimidazole%20AND%20humans)]

Human studies using [^18^F]FETNIM-PET have been performed on head-and-neck cancer (HNC) patients. Those investigations have largely been carried out by researchers at the University of Turku, Finland (7-9). For those studies, a dynamic PET imaging was used in combination with measurements of blood flow using [^15^O]H_2_O (median dose:1,152 MBq (31.1 mCi); dose range: 1,014 -1,800 MBq (27.4 - 48.6 mCi)) and blood volume using [^15^O]CO (median dose: 2,699 MBq (72.9 mCi); dose range: 2,496 - 2,992 MBq (67.4 - 80.8 mCi)). In one reported study using eight untreated HNC patients (7), the tumor blood flow observed was 5 to 30 times greater than in muscle, in contrast to blood volume which remained identical in the two tissues. The tumor distribution volume (calculated using the graphic analysis applied by Logan et al. (10), except for the early phase of [^18^F]FETNIM peak activity) correlated strongly with the standardized uptake value (SUV) of [^18^F]FETNIM between 60 and 120 min, and with blood flow. The highest correlation was obtained at 90 min (r^2^ = 0.935; P < 0.0001).

In a study by Tolvanen et al. (9) using intravenous injections of [^18^F]FETNIM on HNC patients (mean activity 366 MBq), the reported effective dose to a 70-kg adult was 0.015 or 0.019 mSv/MBq, for a 2- and 4-h voiding intervals. The critical organ with the highest absorbed dose was the urinary bladder wall (0.062 and 0.127 mGy/MBq for a 2-h and 4-h intervals). Absorbed doses in all other organs were at least five times smaller than the bladder wall dose (e.g. 0.006 and 0.014 mGy/MBq for the brain and gallbladder wall respectively, at 2-h and 4-h intervals. With an injected activity of 370 MBq (100mCi), the radiation doses were found generally comparable to those of other related radionuclide imaging procedures.

## References

1 Nunn A, Linder K, Strauss HW. (1995). Nitroimidazoles and imaging hypoxia. Eur J Nucl Med.
2 Hodgkiss RJ. (1998). Use of 2-nitroimidazoles as bioreductive markers for tumour hypoxia. Anticancer Drug Des.
3 Yang DJ, Wallace S, Cherif A, Li C, Gretzer MB, Kim EE, Podoloff DA. (1995). Development of F-18-labeled fluoroerythronitroimidazole as a PET agent for imaging tumor hypoxia. Radiology.
4 Gronroos T, Eskola O, Lehtio K, Minn H, Marjamaki P, Bergman J, Haaparanta M, Forsback S, Solin O. (2001). Pharmacokinetics of [18F]FETNIM: a potential marker for PET. J Nucl Med.
5 Rasey JS, Grunbaum Z, Magee S, Nelson NJ, Olive PL, Durand RE, Krohn KA. (1987). Characterization of radiolabeled fluoromisonidazole as a probe for hypoxic cells. Radiat Res.
6 Chung JK, Chang YS, Lee YJ, Kim YJ, Jeong JM, Lee DS, Jang JJ, Lee MC. (1999). The effect of tumor size on F-18-labeled fluorodeoxyglucose and fluoroerythronitroimidazole uptake in a murine sarcoma model. Ann Nucl Med.
7 Lehtio K, Oikonen V, Gronroos T, Eskola O, Kalliokoski K, Bergman J, Solin O, Grenman R, Nuutila P, Minn H. (2001). Imaging of blood flow and hypoxia in head and neck cancer: initial evaluation with [(15)O]H(2)O and [(18)F]fluoroerythronitroimidazole PET. J Nucl Med.
8 Lehtio K, Eskola O, Viljanen T, Oikonen V, Gronroos T, Sillanmaki L, Grenman R, Minn H. (2004). Imaging perfusion and hypoxia with PET to predict radiotherapy response in head-and-neck cancer. Int J Radiat Oncol Biol Phys.
9 Tolvanen T, Lehtio K, Kulmala J, Oikonen V, Eskola O, Bergman J, Minn H. (2002). 18F-Fluoroerythronitroimidazole radiation dosimetry in cancer studies. J Nucl Med.
10 Logan J. (2000). Graphical analysis of PET data applied to reversible and irreversible tracers. Nucl Med Biol.